# ^68^Ga-Labeled 2-[3-(1-carboxy-5-{7-[5-carboxy-5-(3-phenyl-2-{3-phenyl-2-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]propionylamino}propionylamino)pentylcarbamoyl]heptanoylamino}pentyl)ureido]pentanedioic acid

Chemical name: | ^68^Ga-Labeled 2-[3-(1-carboxy-5-{7-[5-carboxy-5-(3-phenyl-2-{3-phenyl-2-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]propionylamino} propionylamino)pentylcarbamoyl]heptanoylamino} pentyl)ureido]pentanedioic acid
Abbreviated name: | [^68^Ga]6
Synonym:
Agent Category: | Compound
Target: | Prostate-specific membrane antigen (PSMA)
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information on [^68^Ga]6 in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=psma%20and%20prostate%20cancer&cmd=DetailsSearch)]

The prostate-specific membrane antigen (PSMA) is a type II membrane glycoprotein that is present primarily in the prostate and is overexpressed during all stages of the androgen-insensitive or the metastatic cancer of this organ (1). In addition, PSMA is expressed at lower levels (compared to the prostate) in the neovasculature of some solid tumors (for details, see Elsasser-Beile et al. (1)). Because of its high expression during the development and progression of a malignancy, PSMA is considered to be a good target for the imaging and treatment of prostate cancer (2). Several investigators have reported the use of radio-halogenated (e.g., ^18^F, ^125^I, etc.) and ^99m^Tc-labeled small molecule inhibitors for the imaging of PSMA (3). Among these radionuclides, ^18^F is the most frequently used to label diverse positron emission tomography (PET) agents for diagnostic imaging because its addition to a molecule (usually by the replacement of a hydrogen atom) does not alter its chemical properties; however, due to its short half-life (~110 min), an on-site cyclotron is needed to produce this radio-halogen (4). Recently ^68^Ga (half-life, ~68 min) has been suggested to be a suitable alternative to the use of ^18^F for the production of PET imaging probes because ^68^Ga is easy to produce with a ^68^Ge/^68^Ga generator system that does not have to be on-site. However, it is necessary to mention that currently no ^68^Ge/^68^Ga generator system has been approved by the United States Food and Drug Administration (Eckelman: personal communication). In addition, ^68^Ga has been successfully used by some investigators to study cancer and tumor biology (4, 5). On the basis of these observations, and as an extension of their earlier work (Banerjee et al. developed two ^68^Ga-labeled, urea-based inhibitors of PSMA ([^68^Ga]-labeled 2-[3-(1-carboxy-5-{7-[5-carboxy-5-(3-phenyl-2-{3-phenyl-2-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]propionylamino}propionylamino)pentylcarbamoyl]

heptanoylamino}pentyl)ureido]pentanedioic acid ([^68^Ga]6)) and [^68^Ga]-labeled 2-{3-[5-(7-{1-benzyloxycarbonyl-5-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]pentylcarbamoyl}-heptanoylamino)-1-carboxypentyl]ureido}pentanedioic acid ([^68^Ga]3)) and evaluated them for biodistribution and the imaging of PSMA-expressing tumors in nude mice (3). This chapter details the results obtained with [^68^Ga]6. Results obtained with [^68^Ga]3 are presented in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Other Sources of Information

PSMA-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=PSMA+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Alternate names and other information regarding PSMA in the Human Protein Reference Database (http://www.hprd.org/alternate?hprd_id=02961&isoform_id=02961_1&isoform_name=Isoform_1).

Clinical trials (http://clinicaltrials.gov/ct2/results?term=PSMA) involving PSMA and PSMA inhibitors.

Gene information (Gene ID: 2346) for human PSMA in Entrez Gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=2346).

PSMA1 variant 3 Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001193471.1).

Information on PSMA in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/600934).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B68Ga%5D3%20synthesis&cmd=DetailsSearch)]

The synthesis of [^68^Ga]6 has been described in detail by Banerjee et al. (3). The radiochemical yield and purity of the labeled compound were reported to be 70.0% and >99.0%, respectively. The retention time of [^68^Ga]6 on analytical high-performance liquid chromatography (HPLC) was 22.5 min compared with a retention time of 25.0 min for [^68^Ga]3. The specific activity of [^68^Ga]6 was reported to be between 3.0 and 6.0 MBq/nmol (81 and 162 μCi/nmol), which was similar to that of [^68^Ga]3. After purification, the radiochemical was dried under vacuum and diluted in 0.9% saline to the desired tracer concentration and used in biodistribution and imaging studies. The stability of [^68^Ga]6 under in vitro or in vivo conditions was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20in%20vitro&cmd=DetailsSearch)]

Using unlabeled 6 and [^68^Ga]6 in a fluorescence-based PSMA inhibition assay, the inhibitory concentrations of these compounds were reported to be 1.23 and 0.44 nM, respectively (3). In comparison, the PSMA inhibitory concentrations for unlabeled 3 and [^68^Ga]3 were 2.9 and 29.0 nM, respectively.

Using a 1-octanol/water mixture with the shake flask method, the partition coefficient of [^68^Ga]6 was determined to be −3.9, which was similar to that of [^68^Ga]3 (3). This indicated that both radiolabeled compounds had a lipophilic nature (3). On the basis of the HPLC analysis reported above, [^68^Ga]6 appeared to have a slightly higher lipophilicity than [^68^Ga]3.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of [^68^Ga]6 was studied in severe-combined immunodeficient (SCID) mice bearing PC-3 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1435&Template=cellBiology)-PIP (transfected with the PSMA gene and expressing high levels of the antigen) and PC-3-FLU (does not express PSMA) cell xenograft tumors (3). The mice were injected with the tracer through the tail vein and euthanized 5, 60, 120, and 180 min after the injection (n = 4 mice/time point) to determine the amount of radioactivity accumulated in the tumors and major organs. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). At 5 min post-injection (p.i.), the PSMA-expressing tumor had an uptake of 6.61 ± 0.55% ID/g that decreased to 1.80 ± 0.16% ID/g by 3 h p.i. Non-targeted organs such as kidneys, spleen, and lungs that contain high levels of PSMA showed a high uptake of 64.75 ± 12.00% ID/g, 5.17 ± 2.22% ID/g, and 4.59 ± 0.68% ID/g, respectively, at 5 min p.i. The radioactivity in these organs dropped to 10.04 ± 1.22% ID/g, 0.34 ± 0.09% ID/g, and 0.14 ± 0.03% ID/g, respectively, at 3 h p.i. Similar to [^68^Ga]3, (see below for details), the clearance of radioactivity with [^68^Ga]6 from the kidneys was faster than from the PSMA-expressing tumors. In mice injected with [^68^Ga]6 PC-3-PIP, the tumor/muscle uptake ratio (T/M) increased from 4.17 at 30 min p.i. to 436.29 at 3 h p.i.; during the same time, the PC-3-FLU tumor T/M ratio increased from 1.67 at 30 min p.i. to 28.70 at 3 h p.i.

A biodistribution study was also performed with [^68^Ga]3 in SCID mice bearing the same tumors as described above (3). At 30 min p.i., the [^68^Ga]3 uptake of the PC-3-PIP tumors decreased gradually from 3.78 ± 0.09% ID/g to 1.10 ± 0.19% ID/g by 3 h p.i. (uptake in the PC-3-FLU tumors was 0.82 ± 0.20% ID/g at 30 min p.i. and 0.39 ± 0.02% ID/g at 3 h p.i.). During the same period, the label cleared rapidly from the kidneys, decreasing from 97.19 ± 16.07% ID/g at 30 min p.i. to 2.13 ± 0.11% ID/g at 3 h p.i. Except for the bladder, all other organs had <1.0% ID/g incorporation of radioactivity by 3 h p.i. The accumulation of radioactivity in the bladder was 8.96 ± 5.30% ID/g at 30 min p.i.; accumulation increased to 25.29 ± 8.63% ID/g at 60 min p.i. and decreased to 5.39 ± 2.98 at 3 h p.i. This indicated that the tracer was excreted mainly through the urinary route. With [^68^Ga]3, the PC-3-PIP T/M increased from 8.30 at 30 min p.i. to 20.37 at 3 h p.i. In comparison, the T/M for the PC-3-FLU tumors was 1.80 at 30 min p.i. and increased to 7.34 at 3 h p.i.

For the PET imaging study, a single animal bearing LNCaP (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1740&Template=cellBiology) cell (expressing PSMA) tumors was injected intravenously with either [^68^Ga]3 or [^68^Ga]6 as described by Banerjee et al. (3). From the PET images it was clear that both tracers accumulated primarily in the PSMA-positive tumors and the kidneys (the kidneys are known to express PSMA in the proximal renal tubules), similar to the observations made during the biodistribution study. In a blocking study, the tumor-bearing mice (the number of animals used per timepoint was not reported) were injected with 2-(phosphonomethyl)pentanedioic acid (2-PMPA) (50 mg/kg body weight), a known selective ligand of PSMA, and later the animals were injected with the respective tracers (time elapsed between the pretreatment with 2-PMPA and injection of the tracer was not reported). PET images of the animals were acquired at 30 and 60 min p.i., and it was observed that the PSMA-expressing tumors and the kidneys did not accumulate either tracer, suggesting that both radiochemicals bound specifically to the membrane antigen.

From these studies, the investigators concluded that both [^68^Ga]3 and [^68^Ga]6 bind specifically to PSMA and could be used for the imaging of PSMA-positive tumors in rodents (3). They also mentioned that more animal studies are necessary before these radiochemicals can be evaluated in the clinic.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were funded by National Institutes of Health grants R01CA134675 and U24 CA92871.

## References

1 Elsasser-Beile U., Buhler P., Wolf P. (2009). Targeted therapies for prostate cancer against the prostate specific membrane antigen. Curr Drug Targets.
2 Dijkgraaf I., Boerman O.C. (2009). Radionuclide imaging of tumor angiogenesis. Cancer Biother Radiopharm.
3 Banerjee S.R., Pullambhatla M., Byun Y., Nimmagadda S., Green G., Fox J.J., Horti A., Mease R.C., Pomper M.G. (2010). 68Ga-labeled inhibitors of prostate-specific membrane antigen (PSMA) for imaging prostate cancer. J Med Chem.
4 Fani M., Andre J.P., Maecke H.R. (2008). 68Ga-PET: a powerful generator-based alternative to cyclotron-based PET radiopharmaceuticals. Contrast Media Mol Imaging.
5 Holland J.P., Williamson M.J., Lewis J.S. (2010). Unconventional nuclides for radiopharmaceuticals. Mol Imaging.
6 Chopra, A., [68Ga]-Labeled 2-{3-[5-(7-{1-Benzyloxycarbonyl-5-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]
pentylcarbamoyl}-heptanoylamino)-1-carboxypentyl]ureido}pentanedioic acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.